# ^99m^Tc-pGlu-Gln-Trp-Ala-Val-Gly-His-Phe-Met-NH2

Chemical name: | ^99m^Tc-pGlu-Gln-Trp-Ala-Val-Gly-His-Phe-Met-NH2
Abbreviated name: | ^99m^Tc-Litorin
Synonym:
Agent Category: | Peptide
Target: | Gastrin-releasing peptide receptor (GRP-R)
Target Category: | Receptor-ligand binding
Method of detection: | SPECT, gamma planar imaging
Source of signal: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=462541) for more information about litorin.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+Litorin)]

Bombesin (BBN or BN)-like peptide is an analog of human gastrin-releasing peptide (GRP) that binds to GRP receptors (GRP-R) (1). Both GRP and BN share an amidated C-terminus sequence homology of seven amino acids (Trp-Ala-Val-Gly-His-Leu-Met-NH_2_). BN peptides induce such biological responses as secretion of adrenal, pituitary, and gastrointestinal hormones; gastric acid secretion; modulation of neuronal firing rate; and regulation of smooth muscle contraction (2, 3). BN-Related peptide receptors can be divided into four subtypes: GRP-R (BB2, BRS-2), neuromedin B receptor (NMB-R, BB1, BRS-1), the orphan receptor BB3-R (BRS-3), and the amphibian receptor BB4-R (1). Several human cancers, such as prostate, breast, lung, colon, and pancreatic cancers, overexpress receptors for BN-like peptides. The BN-like peptides have been radiolabeled with different radionuclides for in vivo imaging of various cancers (4-7).

Litorin (pGlu-Gln-Trp-Ala-Val-Gly-His-Phe-Met-NH_2_), an amphibian BN peptide derivative, is found to stimulate the contraction of smooth muscle, to stimulate gastrin, gastric acid, and pancreatic secretion, and to suppress the nutriment in in vivo experiments (1). ^99m^Tc-Litorin was developed for non-invasive imaging of tumors with overexpressed GRP-R (8).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+Litorin+synthesis)]

Durkan et al. (8) reported the synthesis of ^99m^Tc-litorin by incubation of 5 μg litorin, 25 μg SnCl_2_, and 55.5 MBq (1.5 mCi ) Na[^99m^TcO_4_] (pH 3.0) for 25 min at room temperature. Radiochemical yield was >95%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+Litorin+in+vitro)]

The in vitro solution stability of ^99m^Tc-litorin was tested by incubating the radiolabeled peptide in buffer solution with 500 or 1,000 molar excess of cysteine at 37ºC for 1 h (8). No significant degradation of ^99^Tc-litorin was observed at 500 molar excess of cysteine; 1,000 molar excess of cysteine displaced 16.8 ± 2.7% of radioactivity from litorin, which suggests that the bond strength of ^99m^Tc to litorin is high. Serum stability was 87.4 ± 1.1% at 37ºC for 4 h.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+Litorin+rodentia)]

Durkan et al. (8) performed biodistribution studies of ^99m^Tc-litorin in normal male rats at 30, 90, 180, and 300 min after injection. The organ with the highest accumulation of ^99m^Tc-litorin at 30 min after injection was the pancreas (23.56 ± 0.01% injected dose per gram (% ID/g)), followed by the kidney (11.93 ± 0.8% ID/g), spleen (4.73 ± 0.83% ID/g), prostate (0.41 ± 0.01% ID/g), and liver (0.36 ± 0.08% ID/g). The uptake in the pancreas remained the same at 90 min, whereas the uptake in the kidney, small intestine, and liver increased. ^99m^Tc-Litorin exhibited rapid clearance, as low radioactivity remained in all tissues by 180 and 300 min. ^99m^Tc-Litorin exhibited low hepatobiliary clearance and predominantly renal excretion. Litorin pretreatment resulted in a reduction of radioactivity in the pancreas (98%), spleen (95%), prostate (54%), and small intestine (27%) at 30 min.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+Litorin+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+Litorin+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+Litorin+human)]

No publication is currently available.

## References

1 Ohki-Hamazaki H., Iwabuchi M., Maekawa F. (2005). Development and function of bombesin-like peptides and their receptors. Int J Dev Biol.
2 Rozengurt E., Guha S., Sinnett-Smith J. (2002). Gastrointestinal peptide signalling in health and disease. Eur J Surg Suppl.
3 Roesler R., Henriques J.A., Schwartsmann G. (2006). Gastrin-releasing peptide receptor as a molecular target for psychiatric and neurological disorders. CNS Neurol Disord Drug Targets.
4 Maina T., Nock B., Mather S. (2006). Targeting prostate cancer with radiolabelled bombesins. Cancer Imaging.
5 Smith C.J., Volkert W.A., Hoffman T.J. (2005). Radiolabeled peptide conjugates for targeting of the bombesin receptor superfamily subtypes. Nucl Med Biol.
6 Weiner R.E., Thakur M.L. (2005). Radiolabeled peptides in oncology: role in diagnosis and treatment. BioDrugs.
7 Zhou J., Chen J., Mokotoff M., Ball E.D. (2004). Targeting gastrin-releasing peptide receptors for cancer treatment. Anticancer Drugs.
8 Durkan K., Lambrecht F.Y., Unak P. (2007). Radiolabeling of bombesin-like peptide with 99mTc: 99mTc-litorin and biodistribution in rats. Bioconjug Chem.